# [^99m^Tc(CO)_3_]^+^-Labeled anti-epidermal growth factor receptor (HER2) affibody Z_HER2:342_ with a hexa-histidine tag (H_6_) on the C-terminal

Chemical name: | [^99m^Tc(CO)_3_]^+^-Labeled anti-epidermal growth factor receptor (HER2) affibody Z_HER2:342_ with a hexa-histidine tag (H_6_) on the C-terminal
Abbreviated name: | [^99m^Tc(CO)_3_]^+^-Z_HER2:342_-H_6_
Synonym:
Agent Category: | Affibody (antibody)
Target: | Epidermal growth factor receptor (HER2)
Target Category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=affibody%20zher2%20342&cmd=DetailsSearch)]

Overexpression of the epidermal growth factor receptor type 2 (HER2) is a characteristic feature of a variety of cancers, and HER2 levels in tumors (primary or metastatic) are often used to screen for patients who would benefit from anti-HER2 antibody (Ab) therapy (e.g., for breast cancer), to determine the efficacy of a treatment regimen, or to predict the prognostic outcome for a patient (1). Single-photon emission computed tomography (SPECT) or gamma planar imaging with ^99m^Tc-labeled ligands that target HER2 are often used to detect, diagnose, and develop a treatment regimen for cancers that overexpress this receptor (2). Although many Abs (monoclonal, recombinant, etc.) and their derivatives (single-chain and monovalent or divalent Fab fragments, etc.) have been developed and approved for clinical use for the imaging or radioimmunotherapy of such cancers, these agents have limited efficacy because of their immunogenicity (development of Abs against the anti-HER2 Abs), pharmacokinetic properties (long circulating times), and inability to penetrate deep into tissue (due to the large size of ~150 kDa) (3). Therefore, investigators are constantly developing and evaluating new alternatives to the Ab-based imaging agents (3).

Recently, a small (~7 kDa) Z_HER2:342_ affibody was engineered (4) and labeled with radionuclides such as ^99m^Tc or ^111^In for the detection of HER2-overexpressing tumors with the use of SPECT (2). Later, the affibody and several of its structural derivatives were labeled with ^99m^Tc and used to detect HER2-expressing cancers under preclinical and clinical conditions (for details on the structural derivatives, see Ekblad et al.) (5, 6). It has been shown that a hexa-histidine tag (H_6_; also facilitates purification of the H_6_-bearing compound by immobilized metal ion affinity chromatography) bearing dimeric Z_HER2:342_ could be labeled with ^99m^Tc-tricarbonyl ([^99m^Tc(CO)_3_]^+^) to obtain [^99m^Tc(CO)_3_]^+^-H_6_-(Z_HER2:342_)_2_, and that the radiochemical was suitable to visualize the expression of HER2 in tumor-bearing mice (7). However, for the duration of the study, a higher amount of radioactivity was observed to accumulate in the liver compared to the tumors. From these observations the investigators concluded that, because the liver is often the organ to which a cancer metastasizes, H_6_-(Z_HER2:342_)_2_ was suitable only for the imaging of extrahepatic tumors. Other investigators have also shown that an H_6_ tag located on the N-terminal on a ^99m^Tc-labeled anti-HER2 affibody leads to increased accumulation of label in the hepatic tissue (8, 9). On the basis of a hypothesis that the uptake of the labeled compound by the liver could be reduced by moving the H_6_ tag from the N-terminal of the Z_HER2:342_ affibody or by increasing the hydrophilicity of the tag, two new tracers were constructed by Tolmachev et al. (10). In one construct, the H_6_ tag was moved from the N-terminal of the affibody to the C-terminal to obtain Z_HER2:342_-H_6_; in the second construct, the tag located on the N-terminal of the affibody was made more hydrophilic by alternating glutamic acid residues with the histidines to generate HEHEHE ((HE)_3_) and obtain (HE)_3_-Z_HER2:342_. These constructs were subsequently labeled with [^99m^Tc(CO)_3_]^+^ to form [^99m^Tc(CO)_3_]^+^-Z_HER2:342_-H_6_ and [^99m^Tc(CO)_3_]^+^-(HE)_3_-Z_HER2:342_, respectively. The biodistribution patterns of these radiolabeled affibodies were respectively studied in normal and LS174T (a human colon cancer cell line that has a low expression of HER2) xenograft tumor-bearing nude mice and compared to that of the parent affibody, Z_HER2:342_ (described previously in (11)), which had an H_6_ tag on the N-terminal and was labeled with [^99m^Tc(CO)_3_]^+^ ([^99m^Tc(CO)_3_]^+^-H_6_-Z_HER2:342_). This chapter describes the results obtained with [^99m^Tc(CO)_3_]^+^-Z_HER2:342_-H_6_. Results obtained with [^99m^Tc(CO)_3_]^+^-H_6_-Z_HER2:342_ and [^99m^Tc(CO)_3_]^+^-(HE)_3_-Z_HER2:342_ are described in separate chapters of MICAD (www.micad.nih.gov) and are compared to those obtained with [^99m^Tc(CO)_3_]^+^-Z_HER2:342_-H_6_ (12, 13).

### Other Sources of Information

Affibody Z_HER2:342_ chapters in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=ZHER2+AND+micad%5Bbook%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

Other EGFR imaging agents in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=EGFR+AND+micad%5Bbook%5D&doptcmdl=TOCView&log%24=booksrch&bname=micad).

EGFR (human) ligands (http://www.ncbi.nlm.nih.gov/pubmed?term=Human%20EGFR%20ligands&cmd=DetailsSearch) in PubMed.

Human EGFR in OMIM (http://www.ncbi.nlm.nih.gov/omim?term=Human%20EGFR) (Online Mendelian Inheritance in Man).

Information on EGFR (human) gene (http://www.ncbi.nlm.nih.gov/protein?Db=gene&Cmd=retrieve&dopt=full_report&list_uids=1956&log$=genesensor5&logdbfrom=protein).

Protein (http://www.ncbi.nlm.nih.gov/protein/NP_005219.2?ordinalpos=17&itool=EntrezSystem2.PEntrez.Sequence.Sequence_ResultsPanel.Sequence_RVDocSum) and nucleotide (http://www.ncbi.nlm.nih.gov/nuccore/NG_011529.1?ordinalpos=3&itool=EntrezSystem2.PEntrez.Sequence.Sequence_ResultsPanel.Sequence_RVDocSum) information regarding EGFR.

Anti-EGFR antibody clinical trials (http://clinicaltrials.gov/ct2/results?term=anti-EGFR+antibodies)

EGFR pathways (http://pid.nci.nih.gov/search/intermediate_landing.shtml?molecule=EGFR&Submit=Go) in Pathways Interaction Database

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B99mTc%28CO%293%5D-H6-ZHER2%3A342&cmd=DetailsSearch)]

The production and purification of H_6_-Z_HER2:342_ and its analog Z_HER2:342_-H_6_ were performed as described by Tolmachev et al. (10). The purity values of the two hexa-histidine-linked affibodies were reported to be 98%. The molecular weights of H_6_-Z_HER2:342_ and Z_HER2:342_-H_6_ were reported to be 8.2 kDa and 7873 kDa, respectively. Labeling of the histidine-tagged affibodies with [^99m^Tc(CO)_3_]^+^ is described elsewhere (10). The radiochemical yield and purity of both tracers were 80% and >95%, respectively. The specific activity of the labeled affibodies was 14–15.8 GBq/μmol (378–426 mCi/μmol). Radio-colloid formation in the final preparation of both the radiolabeled affibodies was <1.5% as determined with reversed-phase high-performance liquid chromatography.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20in%20vitro)]

Both [^99m^Tc(CO)_3_]^+^-H_6_-Z_HER2:342_ and [^99m^Tc(CO)_3_]^+^-Z_HER2:342_-H_6_ were reported to be stable in phosphate-buffered saline for at least 24 h at room temperature (23°C). At the end of incubation, 97.2 ± 0.2% and 96.7 ± 0.0% of [^99m^Tc(CO)_3_]^+^-H_6_-Z_HER2:342_ and [^99m^Tc(CO)_3_]^+^-Z_HER2:342_-H_6_, respectively, were reported to be intact as determined with instant thin-layer chromatography (10). A challenge with 500- or 1,000-fold excess histidine for 1 h at 37°C showed that >98% of [^99m^Tc(CO)_3_]^+^-H_6_-Z_HER2:342_ and >95% of [^99m^Tc(CO)_3_]^+^-Z_HER2:342_-H_6_ remained intact at the end of the incubation period. The association equilibrium constant (KD), the association rate constant (Ka), and the dissociation rate constant (Kd) of [^99m^Tc(CO)_3_]^+^-H_6_-Z_HER2:342_ were 23 pM, 4.0 × 10^6^ M^-1^s^-1^, and 8.79 × 10^-5^ s^-1^, respectively, as determined with biosensor analysis. For [^99m^Tc(CO)_3_]^+^-Z_HER2:342_-H_6_, the KD, Ka, and Kd were 20 pM, 2.2 × 10^7^ M^-1^s^-1^, and 4.5 × 10^-4^, respectively.

Using SKOV-3 cells (ovarian cancer cells with high expression of HER2), DU-145 cells, and PC-3 cells (the latter two are prostate cancer cell lines that have a low expression of HER2), the receptor binding specificities of [^99m^Tc(CO)_3_]^+^-H_6_-Z_HER2:342_ were reported to be 48.9 ± 0.8%, 6.1 ± 0.2%, and 6.7 ± 0.1%, respectively; for [^99m^Tc(CO)_3_]^+^-Z_HER2:342_-H_6_, the receptor binding specificities were 46.0 ± 2.0%, 9.0 ± 0.4%, and 6.8 ± 1.0%, respectively (10). Pretreatment of the cells with 100-fold excess unlabeled H_6_-Z_HER2:342_ reduced the receptor binding on the SKOV-3, DU-145, and PC-3 cells significantly (P < 0.0005) to 2.3 ± 0.5%, 3.0 ± 0.3%, and 3.6 ± 0.1%, respectively, for [^99m^Tc(CO)_3_]^+^-H_6_-Z_HER2:342_ and to 3.0 ± 0.1%, 3.1 ± 0.2%, and 3.4 ± 0.2%, respectively, for [^99m^Tc(CO)_3_]^+^-Z_HER2:342_-H_6_. Cellular internalization of [^99m^Tc(CO)_3_]^+^-H_6_-Z_HER2:342_ and [^99m^Tc(CO)_3_]^+^-Z_HER2:342_-H_6_ by the SKOV-3 cells after 24 h incubation at 37°C was determined to be 80.1 ± 0.5% and 47.7 ± 0.1%, respectively. The antigen binding capacity of [^99m^Tc(CO)_3_]^+^-H_6_-Z_HER2:342_ and [^99m^Tc(CO)_3_]^+^-Z_HER2:342_-H_6_ in the presence of 100-fold excess receptor concentration (using intact SKOV-3 cells) was reported to be 79.6 ± 0.6% and 70.3 ± 7.3%, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=H6ZHER2342-99mTc%20rodentia&cmd=DetailsSearch)]

The biodistribution patterns of [^99m^Tc(CO)_3_]^+^-H_6_-Z_HER2:342_ and [^99m^Tc(CO)_3_]^+^-Z_HER2:342_-H_6_ were studied in normal male Naval Medical Research Institute (NMRI) mice (n = 4 animals/time point) after intravenous injection of the respective tracers as described by Tolmachev et al. (10). Accumulated radioactivity in various organs of the animals was determined at 4 h and 24 h postinjection (p.i.) and was presented as percent of injected dose per gram tissue (% ID/g). In the blood, the radioactivity levels of [^99m^Tc(CO)_3_]^+^-H_6_-Z_HER2:342_ and [^99m^Tc(CO)_3_]^+^-Z_HER2:342_-H_6_ were 0.19 ± 0.06% ID/g and 0.9 ± 0.4% ID/g, respectively, at 4 h p.i.; this decreased to 0.07 ± 0.02% ID/g and 0.19 ± 0.04% ID/g, respectively, by 24 h p.i. At 4 h p.i., the kidneys had uptake values of 92.0 ± 23.0% ID/g and 100.0 ± 16.0% ID/g radioactivity from [^99m^Tc(CO)_3_]^+^-H_6_-Z_HER2:342_ and [^99m^Tc(CO)_3_]^+^-Z_HER2:342_-H_6_, respectively. At 24 h p.i., the kidney uptake values had decreased to 45.0 ± 6.0% ID/g and 56.0 ± 10.0%, respectively. In the liver, the accumulations of the label from [^99m^Tc(CO)_3_]^+^-H_6_-Z_HER2:342_ and [^99m^Tc(CO)_3_]^+^-Z_HER2:342_-H_6_ at 4 h p.i. were 10.0 ± 3.0% ID/g and 5.0 ± 1.0% ID/g, respectively, which decreased to 7.0 ± 1.0% ID/g and 2.9 ± 0.5% ID/g, respectively, at 24 h p.i. The spleen showed uptake values of 1.3 ± 0.3% ID/g and 0.8 ± 0.1% ID/g with [^99m^Tc(CO)_3_]^+^-H_6_-Z_HER2:342_ and [^99m^Tc(CO)_3_]^+^-Z_HER2:342_-H_6_, respectively, at 4 h p.i.; by 24 h p.i., the accumulation decreased to 0.8 ± 0.1% ID/g and 0.47 ± 0.07% ID/g, respectively. All other organs showed uptake of <1.0% ID/g radioactivity from the two tracers at both time points. These observations indicated that radioactivity from both tracers was rapidly cleared from the blood and was excreted primarily through the kidneys. The study also showed that, compared to [^99m^Tc(CO)_3_]^+^-H_6_-Z_HER2:342_, approximately two-fold less radioactivity accumulated in the liver with [^99m^Tc(CO)_3_]^+^-Z_HER2:342_-H_6_; however, clearance of the latter tracer from the blood was slower than that of the former (10). The investigators concluded that changing the hexa-histidine tag from the N-terminal to the C-terminal of the affibody had only a small effect on the biodistribution of the molecule. No in vivo blocking studies were reported with either radiolabeled compound.

In another study, the biodistribution patterns of [^99m^Tc(CO)_3_]^+^-H_6_-Z_HER2:342_ and [^99m^Tc(CO)_3_]^+^-Z_HER2:342_-H_6_ were investigated in NMRI nude mice (n = 4 animals) bearing LS174T cell xenograft tumors (10). At 4 h p.i., the accumulations of radioactivity from [^99m^Tc(CO)_3_]^+^-H_6_-Z_HER2:342_ in the kidneys, liver, and the xenograft tumors were 82.0 ± 9.0% ID/g, 8.1 ± 0.8% ID/g, and 2.2 ± 0.3% ID/g, respectively. The tumor/blood (T/B), tumor/liver (T/L), tumor/kidney (T/K), and the tumor/muscle (T/M) ratios with this tracer were 4.5 ± 0.1, 0.29 ± 0.04, 0.028 ± 0.002, and 21.0 ± 0.2, respectively. For [^99m^Tc(CO)_3_]^+^-Z_HER2:342_-H_6_, the label uptake values in the kidneys, liver, and the xenograft tumors were 67.0 ± 13.0% ID/g, 4.3 ± 0.8% ID/g, and 3.2 ± 0.9% ID/g, respectively, and the T/B, T/L, T/K, and T/M ratios were 3.0 ± 0.4, 0.7 ± 0.1, 0.047 ± 0.006, and 17.0 ± 3.0, respectively. This showed that, compared to [^99m^Tc(CO)_3_]^+^-H_6_-Z_HER2:342_, there was a higher uptake of [^99m^Tc(CO)_3_]^+^-Z_HER2:342_-H_6_ by the tumors. This indicated that changing the location of the H_6_ tag from the N-terminal of the affibody to the C-terminal reduced the uptake of radioactivity in the liver and other tissues but increased accumulation of the label in the HER2-positive tumors. No blocking studies with either tracer using the tumor-bearing mice were reported.

Gamma planar imaging of a tumor-bearing mouse showed that the uptake pattern of [^99m^Tc(CO)_3_]^+^-H_6_-Z_HER2:342_ in the animals was similar to that obtained during the biodistribution studies (10). No imaging studies with [^99m^Tc(CO)_3_]^+^-Z_HER2:342_-H_6_ were reported.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=H6ZHER2342-99mTc%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=H6ZHER2342-99mTc%20Non-Human%20Primates&cmd=DetailsSearch)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=H6ZHER2342-99mTc%20Human%20Studies&cmd=DetailsSearch)]

No references are currently available.

## Supplemental Information

[Disclaimers]

No information is currently available

## References

1 Tolmachev V., Rosik D., Wallberg H., Sjoberg A., Sandstrom M., Hansson M., Wennborg A., Orlova A. (2010). Imaging of EGFR expression in murine xenografts using site-specifically labelled anti-EGFR 111In-DOTA-Z EGFR:2377 Affibody molecule: aspect of the injected tracer amount. Eur J Nucl Med Mol Imaging.
2 Orlova A., Feldwisch J., Abrahmsen L., Tolmachev V. (2007). Update: affibody molecules for molecular imaging and therapy for cancer. Cancer Biother Radiopharm.
3 Holliger P., Hudson P.J. (2005). Engineered antibody fragments and the rise of single domains. Nat Biotechnol.
4 Wahlberg E., Lendel C., Helgstrand M., Allard P., Dincbas-Renqvist V., Hedqvist A., Berglund H., Nygren P.A., Hard T. (2003). An affibody in complex with a target protein: structure and coupled folding. Proc Natl Acad Sci U S A.
5 Tolmachev V., Friedman M., Sandstrom M., Eriksson T.L., Rosik D., Hodik M., Stahl S., Frejd F.Y., Orlova A. (2009). Affibody molecules for epidermal growth factor receptor targeting in vivo: aspects of dimerization and labeling chemistry. J Nucl Med.
6 Ekblad T., Orlova A., Feldwisch J., Wennborg A., Karlstrom A.E., Tolmachev V. (2009). Positioning of 99mTc-chelators influences radiolabeling, stability and biodistribution of Affibody molecules. Bioorg Med Chem Lett.
7 Orlova A., Nilsson F.Y., Wikman M., Widstrom C., Stahl S., Carlsson J., Tolmachev V. (2006). Comparative in vivo evaluation of technetium and iodine labels on an anti-HER2 affibody for single-photon imaging of HER2 expression in tumors. J Nucl Med.
8 Ahlgren S., Orlova A., Rosik D., Sandstrom M., Sjoberg A., Baastrup B., Widmark O., Fant G., Feldwisch J., Tolmachev V. (2008). Evaluation of maleimide derivative of DOTA for site-specific labeling of recombinant affibody molecules. Bioconjug Chem.
9 Ahlgren S., Wallberg H., Tran T.A., Widstrom C., Hjertman M., Abrahmsen L., Berndorff D., Dinkelborg L.M., Cyr J.E., Feldwisch J., Orlova A., Tolmachev V. (2009). Targeting of HER2-expressing tumors with a site-specifically 99mTc-labeled recombinant affibody molecule, ZHER2:2395, with C-terminally engineered cysteine. J Nucl Med.
10 Tolmachev V., Hofstrom C., Malmberg J., Ahlgren S., Hosseinimehr S.J., Sandstrom M., Abrahmsen L., Orlova A., Graslund T. (2010). HEHEHE-tagged affibody molecule may be purified by IMAC, is conveniently labeled with [(m)Tc(CO)](+), and shows improved biodistribution with reduced hepatic radioactivity accumulation. Bioconjug Chem.
11 Orlova A., Magnusson M., Eriksson T.L., Nilsson M., Larsson B., Hoiden-Guthenberg I., Widstrom C., Carlsson J., Tolmachev V., Stahl S., Nilsson F.Y. (2006). Tumor imaging using a picomolar affinity HER2 binding affibody molecule. Cancer Res.
12 Chopra, A., [99mTc(CO)3]+-Labeled anti-epidermal growth factor receptor (HER2) affibody ZHER2:342 with a hexa-histidine tag (H6) on the N-terminal. Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
13 Chopra, A., [99mTc(CO)3]+-Labeled anti-epidermal growth factor receptor (HER2) affibody ZHER2:342 with a hexa-histidine tag (H6) on the C-terminal. Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.